# ^111^In-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-NDECELCVNVACTGCL

Chemical name: | ^111^In-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid- NDECELCVNVACTGCL
Abbreviated name: | ^111^In-DOTA-E^3^-uroguanylin
Synonym:
Agent category: | Peptide
Target: | Receptor guanylate cyclase C (GC-C)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/AAC51729.1?ordinalpos=4&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/BC093781.1?ordinalpos=2&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=2981) for more information about uroguanylin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20uroguanylin)]

Receptor guanylate cyclase C (GC-C) is a type I transmembrane glycoprotein expressed on intestinal brush border membranes of intestinal epithelial cells and transformed human colon cancer cell lines (e.g., T84) (1). GC-C is expressed in very low levels on the other tissues and is highly expressed on the primary and metastatic colon cancer tissues (2). Peptides such as the Escherichia coli heat-stable enterotoxin (STh) and uroguanylin have been shown to inhibit the growth of colorectal cancer (CRC) cells in animal models (3-5). STh and uroguanylin are agonistic for the GC-C receptor with nanomolar affinity, resulting in activation of the guanylyl cyclase that increases the intracellular concentration of guanosine 3,5-cyclic monophosphate. Uroguanylin and guanylin are endogenous peptides, which are secreted into the lumen of the gut by enterochromaffin cells to regulate ion and fluid homeostasis (6). However, their expression is lost during cancer transformation (5, 7).

CRC is the second most common type of cancer in the United States (8). The United States Food and Drug Administration (FDA) has approved scintigraphic agents that are based on monoclonal antibodies (mAbs) for the imaging of colorectal cancers (9), but these agents have limitations because of a lack of penetration in tumors and prolonged blood circulation as a result of their large molecular size. Furthermore, the pharmacokinetics of intact radiolabeled mAbs, with high liver uptake and slow blood elimination, are generally not ideal for imaging. 1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid (DOTA) derivatives of STh have been evaluated for in vivo imaging in nude mice bearing colorectal xenografts (10-12). Uroguanylin (NDDCELCVNVACTGCL) is a 16 amino acid peptide with two disulfide bonds and is less complex than STh, which contains three disulfide bonds. The N-terminal end of uroguanylin and E^3^-uroguanylin (NDECELCVNVACTGCL) was conjugated with DOTA for ^111^In-radiolabeling. ^111^In-DOTA-uroguanylin and ^111^In-DOTA-E^3^-uroguanylin have been evaluated in nude mice bearing human colon adenocarcinoma tumors (13).

### Related Resource Links:

- Gene information in NCBI (Guanylate cyclase C (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2984))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=601330)
- Clinical trials (Colorectal cancers (http://www.clinicaltrials.gov/ct2/results?term=colorectal+cancer+imaging))
- FDA Drug information (Colorectal cancer scintigraphy imaging agents (http://google2.fda.gov/search?q=scintigraphy+colon+cancer&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20uroguanylin%20and%20synthesis)]

N-Hydroxysuccinimide (NHS) ester of DOTA (NHS-DOTA) was used in a 100-fold excess to conjugate the N-terminal end of uroguanylin and E^3^-uroguanylin to form DOTA-uroguanylin and DOTA-E^3^-uroguanylin after being incubated overnight at 4°C (13). DOTA-uroguanylin and DOTA-E^3^-uroguanylin were isolated with high-performance liquid chromatography (HPLC) and identified with mass spectroscopy. There was one DOTA molecule per peptide. DOTA-uroguanylin or DOTA-E^3^-uroguanylin (24 nmol) was mixed with 7.5–92.5 MBq (0.2–2.5 mCi) ^111^InCl_3_ and incubated for 60 min at 37°C. ^111^In-DOTA-uroguanylin and ^111^In-DOTA-E^3^-uroguanylin were purified with HPLC. The labeling yield and the radiochemical purity were not reported. The specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20uroguanylin%20and%20in%20vitro)]

The binding affinities of uroguanylin, DOTA-uroguanylin, E^3^-uroguanylin, and DOTA-E^3^-uroguanylin for GC-C were determined using T84 cells (13). In this assay, ^125^I-F19-STh(1-19) was incubated with 3 × 10^6^ cells in the presence of 0.1–1,000 nM corresponding peptide for 60 min at 37°C. The 50% inhibition concentration (IC_50_) values were 39.9, 34.5, 5.0, and 9.6 nM for uroguanylin, DOTA-uroguanylin, E^3^-uroguanylin, and DOTA-E^3^-uroguanylin, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20uroguanylin%20and%20rodentia)]

Liu et al. (13) performed ex vivo biodistribution studies of ^111^In-DOTA-E^3^-uroguanylin and ^111^In-DOTA- uroguanylin (7.4 MBq (0.2 μCi)) in SCID mice (n = 4/group) bearing T84 xenografts. Accumulation levels of the two tracers in the T84 tumors were 1.04 ± 0.07% injected dose per gram (ID/g) and 0.88 ± 0.33% ID/g at 1 h after injection, respectively. The radioactivity levels in tumors were higher than in other organs and tissues (e.g., the lung, liver, spleen, and intestines) except the kidneys (28% ID/g) at 1 h after injection. Blood levels were 0.2–0.4% ID/g at 1 h. Tumor/blood, tumor/muscle, and tumor/liver ratios for ^111^In-DOTA-E^3^-uroguanylin at 1 h after injection were 5, 21, and 6, respectively. These ratios were 61, 61, and 4 at 4 h after injection, respectively. Co-injection of ^111^In-DOTA-E^3^-uroguanylin with E^3^-uroguanylin reduced the radioactivity levels in the tumors and kidneys by 60–70% at 1 h after injection, whereas little inhibition was observed in other tissues. As a comparison with ^111^In-DOTA-R^1,4^-F19-STh(1-19), the kidney uptake of ^111^In-DOTA-E^3^-uroguanylin was ~10-fold greater than that of ^111^In-DOTA-R^1,4^-F19-STh(1-19) at 1 h after injection (12).

Single-photon emission computed tomography analysis was performed in nude mice bearing the T84 tumors after injection of 7.4 MBq (0.2 μCi) ^111^In-DOTA-E^3^-uroguanylin. The tumors were clearly visualized at 1 h along with the kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20uroguanylin%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20uroguanylin%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20uroguanylin%20and%20human)]

No publication is currently available.

## NIH Support

P50 CA103130-01

## References

1 Birbe R., Palazzo J.P., Walters R., Weinberg D., Schulz S., Waldman S.A. (2005). Guanylyl cyclase C is a marker of intestinal metaplasia, dysplasia, and adenocarcinoma of the gastrointestinal tract. Hum Pathol.
2 Ciocca V., Bombonati A., Palazzo J.P., Schulz S., Waldman S.A. (2009). Guanylyl cyclase C is a specific marker for differentiating primary and metastatic ovarian mucinous neoplasms. Histopathology.
3 Li P., Schulz S., Bombonati A., Palazzo J.P., Hyslop T.M., Xu Y., Baran A.A., Siracusa L.D., Pitari G.M., Waldman S.A. (2007). Guanylyl cyclase C suppresses intestinal tumorigenesis by restricting proliferation and maintaining genomic integrity. Gastroenterology.
4 Lin J.E., Li P., Pitari G.M., Schulz S., Waldman S.A. (2009). Guanylyl cyclase C in colorectal cancer: susceptibility gene and potential therapeutic target. Future Oncol.
5 Shailubhai K., Yu H.H., Karunanandaa K., Wang J.Y., Eber S.L., Wang Y., Joo N.S., Kim H.D., Miedema B.W., Abbas S.Z., Boddupalli S.S., Currie M.G., Forte L.R. (2000). Uroguanylin treatment suppresses polyp formation in the Apc(Min/+) mouse and induces apoptosis in human colon adenocarcinoma cells via cyclic GMP. Cancer Res.
6 Greenberg R.N., Hill M., Crytzer J., Krause W.J., Eber S.L., Hamra F.K., Forte L.R. (1997). Comparison of effects of uroguanylin, guanylin, and Escherichia coli heat-stable enterotoxin STa in mouse intestine and kidney: evidence that uroguanylin is an intestinal natriuretic hormone. J Investig Med.
7 Cohen M.B., Hawkins J.A., Witte D.P. (1998). Guanylin mRNA expression in human intestine and colorectal adenocarcinoma. Lab Invest.
8 Levin B., Lieberman D.A., McFarland B., Andrews K.S., Brooks D., Bond J., Dash C., Giardiello F.M., Glick S., Johnson D., Johnson C.D., Levin T.R., Pickhardt P.J., Rex D.K., Smith R.A., Thorson A., Winawer S.J. (2008). Screening and surveillance for the early detection of colorectal cancer and adenomatous polyps, 2008: a joint guideline from the American Cancer Society, the US Multi-Society Task Force on Colorectal Cancer, and the American College of Radiology. Gastroenterology.
9 Wu A.M., Olafsen T. (2008). Antibodies for molecular imaging of cancer. Cancer J.
10 Gali H., Sieckman G.L., Hoffman T.J., Owen N.K., Chin D.T., Forte L.R., Volkert W.A. (2001). In vivo evaluation of an 111In-labeled ST-peptide analog for specific-targeting of human colon cancers. Nucl Med Biol.
11 Giblin M.F., Gali H., Sieckman G.L., Owen N.K., Hoffman T.J., Volkert W.A., Forte L.R. (2006). In vitro and in vivo evaluation of 111In-labeled E. coli heat-stable enterotoxin analogs for specific targeting of human breast cancers. Breast Cancer Res Treat.
12 Giblin M.F., Sieckman G.L., Watkinson L.D., Daibes-Figueroa S., Hoffman T.J., Forte L.R., Volkert W.A. (2006). Selective targeting of E. coli heat-stable enterotoxin analogs to human colon cancer cells. Anticancer Res.
13 Liu D., Overbey D., Watkinson L.D., Daibes-Figueroa S., Hoffman T.J., Forte L.R., Volkert W.A., Giblin M.F. (2009). In vivo imaging of human colorectal cancer using radiolabeled analogs of the uroguanylin peptide hormone. Anticancer Res.